# ^18^F-Labeled Cys-Z_HER2:342_, an anti-epidermal growth factor receptor-2 Affibody

Chemical name: | ^18^F-Labeled Cys-Z_HER2:342_, an anti-epidermal growth factor receptor-2 Affibody
Abbreviated name: | [^18^F]-Cys-Z_HER2:342_
Synonym: | [^18^F]-Z_HER2:342_
Agent Category: | Antibody
Target: | Epidermal growth factor receptor 2 (HER2)
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=affibodies&cmd=DetailsSearch)]

The epidermal growth factor receptor-2 (HER2, ErbB2) modulates its activity through a tyrosine kinase signaling pathway and is involved in the development of various cancers, including those of the lung and the breast (1, 2). Overexpression or amplification of the HER2 gene is known to occur in a high percentage of cancer cases (e.g., ~20% of breast cancer (BC)) and predicts a poor prognosis for the patient. Invasive methods such as biopsies in conjunction with immunohistochemistry and fluorescence in situ hybridization are often employed to assess the HER2 status of the primary and metastasized neoplastic tumors; however, because of sampling bias and tumor heterogeneity, results obtained with these procedures may not be reliable (2). In the clinic, ^18^F-labeled fluorodeoxyglucose ([^18^F]-FDG) is commonly used with positron emission tomography (PET) to detect and determine the tumor burden of a patient, but this technique does not distinguish between benign and malignant lesions, cannot differentiate tumors that overexpress HER2 from those that have a low expression or do not express the receptor, and often identifies inflammation as a false-positive neoplasm (1).

An Affibody molecule is a chain of 58 amino acids (~6.5 kDa) that contains a modified B domain of the staphylococcal protein A and can be obtained by chemical synthesis or produced in bacteria with the use of recombinant DNA technology (3). Because of their small size and high chemical and thermal stability, there is much interest to radiolabel these molecules and use them for the targeted detection and treatment of malignant tumors as discussed in detail elsewhere (3-5). Orlova et al. generated an anti-EGFR2 Affibody molecule (Z_HER2:342_) with a picomolar affinity for the receptor and showed that ^125^I-labeled Z_HER2:342_ can be used to visualize xenograft SKOV-3 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-77&Template=cellBiology) cell tumors (these cells express the HER2) with gamma planar imaging in mice (6). Kramer-Marek et al. envisioned that, because ^18^F is routinely available in the clinic, ^18^F-labeled Z_HER2:342_ can be used to detect and monitor (after therapy) cancerous lesions that express HER2 (7). For the site-specific labeling of Z_HER2:342_ with ^18^F, a cysteine residue was attached to the C-terminus of the Affibody (Cys-Z_HER2:342_), and the derivative was conjugated with N-(2-(4-[^18^F]fluorobenzamido)ethyl)maleimide ([^18^F]FBEM) to obtain [^18^F]-Cys-Z_HER2:342_ (7). Subsequently, the radiofluorinated conjugate was characterized in vitro and evaluated in vivo to assess the expression of HER2 in xenograft tumors in mice (7).

### Related Resource Links

Anti-HER2 affibodies in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Anti-HER2+affibody+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

HER2 clinical trials (http://clinicaltrials.gov/ct2/results?term=HER2)

Other EGFR-imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad)

EGFR (human) ligands (http://www.ncbi.nlm.nih.gov/pubmed?term=Human%20EGFR%20ligands&cmd=DetailsSearch) in PubMed

Human EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Human%20EGFR) (Online Mendelian Inheritance in Man database)

Information on EGFR (human) gene (http://www.ncbi.nlm.nih.gov/protein?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=genesensor5&logdbfrom=protein)

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_005219.2?ordinalpos=17&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NG_011529.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) information regarding EGFR

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F%20cys%20zher2%20342%20synthesis&cmd=DetailsSearch)]

The expression of Z_HER2:342_ in Escherichia coli as a His-tagged protein and its purification from the microbes are described elsewhere (6). The Affibody was labeled with [^18^F]FBEM as detailed by Kiesewetter et al. (8). The radiochemical yield of the labeling reaction was 10.5 ± 1.9% (n = 39 reactions; average time was 117 min/reaction), and the specific activity of the labeled Affibody was 2.51 ± 0.92 MBq/153.8 pmol (93.0 ± 34.2 μCi/153.8 pmol). The radiochemical purity and stability of the labeled product was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F%20cys%20zher2%20342%20in%20vitro&cmd=DetailsSearch)]

The affinity constant (KD), the association rate constant (k_a_), and the dissociation rate constant (k_d_) of Z_HER2:342_ for HER2 were reported to be ~22 pmol/L, ~4.8 × 10^6^ M^–1^s^–1^, and ~1.1 × 10^–4^s^–1^, respectively, as determined with surface plasmon resonance techniques (6).

The in vitro binding characteristics of [^18^F]-Cys-Z_HER2:342_ were studied with displacement and saturation cell-binding assays using SKOV-3 cells (7). For the displacement assay, the cells were incubated with 216 nM [^18^F]-Cys-Z_HER2:342_ in the presence of increasing concentrations of the non-radiolabeled Affibody (1.2 nM–120 μM). This study demonstrated that increasing concentrations of the unlabeled Affibody could displace [^18^F]-Cys-Z_HER2:342_ from the receptor expressed on the SKOV-3 cells (7). The KD of [^18^F]-Cys-Z_HER2:342_ for the HER2 expressed on the SKOV-3 cells was reported to be 15 nM as determined with the saturation binding assay (7).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F%20cys%20zher2%20342%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^18^F]-Cys-Z_HER2:342_ was investigated in mice bearing BT474 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-20&Template=cellBiology) cell tumors (these cells originate from human mammary gland ductal carcinoma) (8). The animals (n = 4–5 anesthetized mice) were injected with 5.5–6.3 MBq (203.5–233.1 μCi; 461.4–633.2 pmol) of the labeled Affibody through the tail vein and euthanized at 2 h postinjection (p.i.). All organs of interest, including the tumors, were harvested from the animals to determine the amount of radioactivity accumulated in the various tissues. Results obtained from this study were calculated as the percent of injected dose per gram tissue (% ID/g). Maximum uptake of label was observed in the tumors (23% ID/g), followed by the kidneys (10% ID/g). All other organs showed an accumulation of <5% ID/g. No blocking studies were reported.

For imaging studies, the anesthetized mice (n = 5 animals) were injected with [^18^F]-Cys-Z_HER2:342_ as described above, and whole-body PET scans of the animals were acquired at 1 h p.i (8). Regions-of-interest (ROI) were marked on the images, and the accumulation values for the various tissues and the tumors were calculated as detailed elsewhere (8). From the images it was apparent that maximum accumulation of label was in the tumors, followed by the kidneys. An analysis of the ROI data showed that the tumor/muscle ratio was 22, and the background activity in the other tissues was very low. From this study, the investigators concluded that the tracer can be used for the detection of HER2-positive tumors. No blocking studies were reported.

Kramer-Marek et al. studied the biodistribution of [^18^F]-Cys-Z_HER2:342_ in athymic nude mice bearing xenograft SKOV-3 cell tumors to assess the utility of this labeled Affibody to monitor the expression of HER2 in cancerous tumors (7). For the biodistribution studies, the mice (n = 3–6 animals/time point) were injected with 1.8–2.2 MBq (66.6–81.4 μCi; 245.3–306.6 pmol) [^18^F]-Cys-Z_HER2:342_, and the animals were euthanized at time points ranging from 1 h p.i. to 6 h p.i. The blood, tumors, and various organs were subsequently collected from the animals to determine the uptake of radioactivity in the different tissues. The amount of radioactivity present in select tissues at select time points is presented in Table 1.

Table 1: Biodistribution of radioactivity from [ ^ 18 ^ F]-Cys-Z _ HER2:342 _ in select tissues at select time points in mice bearing xenograft SKOV-3 cell tumors ( 7 ).

Tissue | Accumulated radioactivity (% ID/g)
Tissue | Time points (p.i.)
Tissue | 1 h | 3 h | 6 h
Blood | 1.31 ± 0.75 | 0.25 ± 0.09 | 0.16 ± 0.08
Kidney | 14.08 ± 0.05 | 2.36 ± 0.11 | 1.43 ± 0.29
Tumor | 9.73 ± 1.91 | 6.95 ± 0.93 | 6.80 ± 0.01
Liver | 5.04 ± 0.69 | 0.68 ± 0.18 | 0.41 ± 0.05
Bone | 2.15 ± 0.40 | 2.07 ± 2.27 | 0.60 ± 0.04

From the biodistribution study, it was apparent that at 6 h p.i. maximum radioactivity was present in the tumors, and all other organs, except the kidneys, accumulated <1.0% ID/g of radioactivity (Table 1). At 4 h p.i., the tumor/blood, tumor/kidney, tumor/bone, and tumor/muscle ratios were 69 ± 27, 4 ± 0.8, 5 ± 2.6, and 311 ± 167, respectively. To establish the in vivo receptor binding specificity of [^18^F]-Cys-Z_HER2:342_, the animals (n = 3–6 mice/group) bearing SKOV-3 cell tumors were injected with 6.1 nmol unlabeled Cys-Z_HER2:342_ 45 min before the administration of [^18^F]-Cys-Z_HER2:342_ (7)_._ For use as controls, another group of mice bearing U251 cell tumors (these cells do not express HER2) were injected with [^18^F]-Cys-Z_HER2:342_ alone. At 2 h p.i., the animals were euthanized, and all the organs of interest, as well as the tumors, were removed to determine the amount of label accumulated in the various tissues. A significantly reduced accumulation of label was observed in the tumors of animals given a blocking dose of unlabeled Cys-Z_HER2:342_ (~6.5% ID/g in mice without blocking versus ~2.0% ID/g in blocked animals; P value not reported). All other organs showed almost no change in uptake of the label. This showed that the ^18^F-labeled Affibody had a binding specificity for the HER2 expressed primarily in the SKOV-3 cell tumors. Pre-incubation with trastuzumab (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=492dbdb2-077e-4064-bff3-372d6af0a7a2) did not inhibit the binding of [^18^F]-Cys-Z_HER2:342_ to the SKOV-3 cells, indicating that the two agents targeted distinctly separate epitopes on the extracellular domain of the HER2 (7).

It has been observed that [^18^F]-Cys-Z_HER2:342_ is superior to [^18^F]-FDG as a tracer for the detection of breast cancer tumors and for the evaluation of the HER2 status of metastasized lesions (1). In another study, it was shown that [^18^F]-Cys-Z_HER2:342_ can be used with PET to determine the changes in the expression of HER2 in BT474 xenografts tumors in mice, and the investigators suggested that determination of the HER2 levels of a tumor may be a good strategy to predict the response of a cancerous lesion to treatment with trastuzumab (2).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F%20cys%20zher2%20342%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F%20cys%20zher2%20342%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=18F%20cys%20zher2%20342%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

Studies reported in this chapter were funded in part by contracts from N01-CO-12400, N01-CO-12401, and HHSN261200800001E from the National Cancer Institute (NCI), National Institutes of Health (NIH). The research was also supported by the Center for Cancer Research, an Intramural Research Program of the NCI, Imaging Probe Development Center, National Heart, Lung and Blood Institute, National Institute of Biomedical Imaging and Bioengineering, NIH.

## References

1 Kramer-Marek G., Bernardo M., Kiesewetter D.O., Bagci U., Kuban M., Omer A., Zielinski R., Seidel J., Choyke P., Capala J. (2012). PET of HER2-Positive Pulmonary Metastases with 18F-ZHER2:342 Affibody in a Murine Model of Breast Cancer: Comparison with 18F-FDG. J Nucl Med.
2 Kramer-Marek G., Gijsen M., Kiesewetter D.O., Bennett R., Roxanis I., Zielinski R., Kong A., Capala J. (2012). Potential of PET to predict the response to trastuzumab treatment in an ErbB2-positive human xenograft tumor model. J Nucl Med.
3 Feldwisch J., Tolmachev V., Lendel C., Herne N., Sjoberg A., Larsson B., Rosik D., Lindqvist E., Fant G., Hoiden-Guthenberg I., Galli J., Jonasson P., Abrahmsen L. (2010). Design of an optimized scaffold for affibody molecules. J Mol Biol.
4 Lofblom J., Feldwisch J., Tolmachev V., Carlsson J., Stahl S., Frejd F.Y. (2010). Affibody molecules: engineered proteins for therapeutic, diagnostic and biotechnological applications. FEBS Lett.
5 Tolmachev V., Orlova A. (2010). Influence of labelling methods on biodistribution and imaging properties of radiolabelled peptides for visualisation of molecular therapeutic targets. Curr Med Chem.
6 Orlova A., Magnusson M., Eriksson T.L., Nilsson M., Larsson B., Hoiden-Guthenberg I., Widstrom C., Carlsson J., Tolmachev V., Stahl S., Nilsson F.Y. (2006). Tumor imaging using a picomolar affinity HER2 binding affibody molecule. Cancer Res.
7 Kramer-Marek G., Kiesewetter D.O., Martiniova L., Jagoda E., Lee S.B., Capala J. (2008). [18F]FBEM-Z(HER2:342)-Affibody molecule-a new molecular tracer for in vivo monitoring of HER2 expression by positron emission tomography. Eur J Nucl Med Mol Imaging.
8 Kiesewetter D.O., Kramer-Marek G., Ma Y., Capala J. (2008). Radiolabeling of HER2 specific Affibody(R) molecule with F-18. J Fluor Chem.